# ^111^In-Streptavidin-biotinylated α-melanocyte-stimulating hormone 2.0 bacteriophage

Chemical name: | ^111^In-Streptavidin-biotinylated α-melanocyte-stimulating hormone 2.0 bacteriophage
Abbreviated name: | ^111^In-SA-α-MSH2.0 phage
Synonym: | Pretargeted ^111^In-MSH bacteriophage
Agent Category: | Bacteriophage
Target: | Melanocortin-1 (MC-1) receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal/contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=4157) for more information about the melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-SA-MSH2.0%20phage%29%20OR%20%28pretargeted%20bivalent%20bacteriophage%29)]

^111^In-Streptavidin-biotinylated α-melanocyte-stimulating hormone (MSH) 2.,0 bacteriophage (^111^In-SA-α-MSH2.0 phage) is a two-step melanoma pretargeting and imaging system developed as a single-photon emission computed tomography (SPECT) imaging probe for primary and metastatic melanoma (1). This system uses a biotinylated α-MSH2.0 (bio-MSH2.0) targeting phage combined with in vivo labeling by ^111^In-streptavidin (^111^In-SA).

Malignant melanoma is the sixth most common cancer in the United States (2). Early diagnosis and prompt surgical removal comprise the best approach for treatment (3). The melanocortin (MC) system is the best characterized neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (4). Most cutaneous cell types express MC receptors, proopiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Five MC receptors (MC-1 to MC-5) have been cloned and characterized as receptors that belong to the G-protein−coupled receptor superfamily. MSHs (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), composed of 13 amino acids, is the most potent naturally occurring melanotropic peptide (5). The biological effects of α-MSH are mediated via MC receptors.

Although positron emission tomography imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (6, 7). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC-1 receptors that are overexpressed on human and mouse melanoma cells (6, 8-11). To improve the in vivo pharmacokinetics of these radiolabeled peptides, different α-MSH analogs have been designed and studied (12, 13). Bacteriophage display (phage display) is a combinatorial chemistry technique that uses a population of filamentous bacteriophage particles genetically modified to display a library of proteins and peptides on their surface (14, 15). This technique has been used for the discovery of new and unique molecular imaging peptides (16). These phage display–derived peptides can have binding properties different from chemically synthesized peptides because the conformational structures of phage peptides are affected by the microenvironment created by the surface of the phage particle (1). Instead of using the isolated peptides, Newton et al. (1) suggested that imaging tags can be directly added to phage particles without significant effects on their peptide binding properties. However, these very high molecular weight phage particles are generally cleared by the reticuloendothelial system in vivo. To circumvent this problem, Newton et al. (1) prepared an α-MSH2.0 peptide analog from the phage display library and proposed the use of a two-step biotin-SA pretargeting system to allow for clearance of unlabeled phage particles before injection of the ^111^In imaging label.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pretargeted%20bivalent%20bacteriophage)]

The α-MSH2.0 phage was generated by use of the fUSE5 vector, which contained phage with modified coat protein III and displayed up to 5 copies of a fused peptide on the tip of the phage particle (1). Affinity selection of phage constructs was performed through multiple rounds of washing and multiplication. Briefly, the fUSE5 vector was digested with the SFiI restriction endonuclease. Equal molar amounts of sense and antisense phosphorylated DNA oligonucleotides were hybridized. A room-temperature DNA ligation reaction was performed for insertion of the hybridized DNA into the fUSE5 vector. Escherichia coli K91 Blue Kan cells were electroporated in the presence of the ligated vector. The proper DNA sequence was verified by DNA sequencing, and the amplified phage was precipitated. The phage particle concentrations in virions were determined spectrophotometrically.

Biotinylation of the phage particle was conducted by adding commercially available NHS-PEO_4_-biotin to the phage suspension at a 1,000-fold molar excess relative to the phage particles (1). The mixture was rotated at room temperature for 2 h. The reaction was stopped with ethanolamine (pH 9.0) and was rotated at room temperature for 1 h. The free biotin was removed from bio-MSH2.0 by dialysis. ^111^In-SA was prepared by first attaching diethylenetriaminepentaacetic acid (DTPA) to SA molecules. This was performed by mixing 2-(4-isothiocyanatobenzyl)-DTPA in carbonate buffer (pH 9.5) with SA suspension at a 50-fold molar excess of DTPA. The mixture was rotated overnight at 4ºC. After removal of excess DTPA, DTPA-SA was radiolabeled with ^111^In by incubation with ^111^In chloride in 10 mM N-(2-hydroxyethyl)piperazine-N'-(2-ethanesulfonic acid (HEPES, pH 7.0) at 37ºC for 1.5 h. Free ^111^In was removed by Zeba Desalt Spin Columns. The specific activity and radiochemical purity of ^111^In-SA were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28pretargeted%20bivalent%20bacteriophage%29%20AND%20in%20vitro)]

Newton et al. (1) conducted phage sequencing to confirm that the MSH2.0 phage clone contained a modified α-MSH sequence. MSH2.0 lacked 3 nonessential amino acids at the amino terminus of the α-MSH sequence and contained a linker peptide between it and the phage coat protein III (NH_2_-AMEHFRWGRPVGSGSGSGSVWYAG-coat protein III). The phase clones were then probed with an anti–α-MSH antibody to determine whether the peptide sequences were accessible and reactive with the MC-1 receptor. The phage particle dot blot assay showed that the α-MSH sequence on the MSH2.0 phage clone was immunoreactive. A micropanning assay with B16/F1 mouse melanoma cells was performed to test the specific binding of MSH2.0 phage. The results indicated specific binding of MSH2.0 peptide to B16/F1 cells. There was no significant alteration of phage binding in vitro with the addition of PEO_4_-biotin to the surface of the phage particle.

The DTPA-SA complex was prepared with >90% labeling efficiency (1). An in vitro stability test showed that ^111^In-SA retained 100% labeling activity in phosphate-buffered saline and HEPES for at least 24 h at 25ºC and 37ºC. ^111^In-SA retained ~80% activity when incubated in mouse serum for 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28pretargeted%20bivalent%20bacteriophage%29%20AND%20rodentia)]

Newton et al. (1) conducted biodistribution studies of the pretargeted bio-MSH2.0 followed by ^111^In-SA in mice bearing B16/F1 mouse melanoma (0.05–0.1 g s.c. tumors). Each mouse received an i.v. injection of 5 × 10^12^ virions of bio-MSH2.0. After 4 h, an i.v. injection of 1.85 MBq (0.05 mCi) ^111^In-SA was administered. ^111^In-SA radioactivity was primarily cleared by the urinary and hepatobiliary systems. The initial tumor radioactivity of ~2.5% injected dose per g (% ID/g; n = 3) appeared to be attributable to the tumor blood volume. After 24 h, there was actual radioactivity retention of 1.0 ± 0.1% ID/g and the tumor/muscle and tumor/blood ratios were 17.5 ± 3.7 and 2.0 ± 0.2, respectively. In comparison, the tumor radioactivity of ^111^In-SA alone without bio-MSH2.0 was 0.4 ± 0.1% ID/g at 24 h. The biotinylated nonspecific wild-type phage tumor radioactivity level was 1.8-fold less than that of bio-MSH2.0 at 24 h. This suggested that the in vivo targeting of ^111^In-SA-α-MSH2.0 phage to the tumor was mediated by α-MSH peptide. Coinjection of bio-MSH2.0 with 100 μg of [NIe^4^,D-Phe^7^]α-MSH (NDP), a potent protease-resistant peptide analog of α-MSH, decreased the tumor radioactivity retention of bio-MSH2.0 by 2.4 ± 0.4-fold. The authors suggested that this demonstrated the specificity of binding for the bio-MSH2.0 phage in vivo.

SPECT imaging of ^111^In-SA–α-MSH2.0 phage was performed in mice bearing B16/F1 mouse melanoma (1). Each mouse received 5 × 10^12^ virions of bio-MSH2.0 and then 7.4 MBq (0.2 mCi) of ^111^In-SA. The study clearly demonstrated the accumulation of ^111^In-SA radioactivity within the tumor. The mice were euthanized 4 h after injection. The tumor radioactivity level at 4 h was 5.2 ± 0.8% ID/g, which was higher than the biodistribution study value of 0.9 ± 0.3% ID/g. The authors suggested that the higher value in the imaging study was attributable to the higher dose of ^111^In-SA administered in the study.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28pretargeted%20bivalent%20bacteriophage%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28pretargeted%20bivalent%20bacteriophage%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28pretargeted%20bivalent%20bacteriophage%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH P50 CA103130-01.

## References

1 Newton J.R., Miao Y., Deutscher S.L., Quinn T.P. (2007). Melanoma imaging with pretargeted bivalent bacteriophage. J Nucl Med.
2 Miao Y., Benwell K., Quinn T.P. (2007). 99mTc- and 111In-labeled alpha-melanocyte-stimulating hormone peptides as imaging probes for primary and pulmonary metastatic melanoma detection. J Nucl Med.
3 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
4 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
5 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
6 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
7 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
8 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
9 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
10 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
11 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
12 Froidevaux S., Calame-Christe M., Tanner H., Eberle A.N. (2005). Melanoma targeting with DOTA-alpha-melanocyte-stimulating hormone analogs: structural parameters affecting tumor uptake and kidney uptake. J Nucl Med.
13 Miao Y., Owen N.K., Whitener D., Gallazzi F., Hoffman T.J., Quinn T.P. (2002). In vivo evaluation of 188Re-labeled alpha-melanocyte stimulating hormone peptide analogs for melanoma therapy. Int J Cancer.
14 Smith G.P. (1985). Filamentous fusion phage: novel expression vectors that display cloned antigens on the virion surface. Science.
15 Koscielska K., Kiczak L., Kasztura M., Wesolowska O., Otlewski J. (1998). Phage display of proteins. Acta Biochim Pol.
16 Chen X., Sievers E., Hou Y., Park R., Tohme M., Bart R., Bremner R., Bading J.R., Conti P.S. (2005). Integrin alpha v beta 3-targeted imaging of lung cancer. Neoplasia.